# [^18^F]Fluoro-[1,2-^2^H_4_]choline

Chemical name: | [^18^F]Fluoro-[1,2-^2^H_4_]choline
Abbreviated name: | [^18^F]12c, D4-FCH
Synonym: | [^18^F]Fluoromethyl-[1,2-^2^H_4_]choline
Agent category: | Compound
Target: | Choline kinases
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine)]

Choline is an important component of phospholipids in cell membranes. Increased metabolism in tissues will lead to an increased uptake of choline. Choline is phosphorylated by choline kinases (CHK) to phosphorylcholine within cells and, after several biosynthetic processes, is finally integrated into phospholipids (1). Because tumor cells have a high metabolic rate, choline uptake is high in order to keep up with the demands of the synthesis of phospholipids in their cellular membranes (2).

Positron emission tomography (PET) with [^11^C]choline (http://www.ncbi.nlm.nih.gov/books/NBK23549/#Choline11C) has been reported to be useful for the detection and differential diagnosis of brain tumors, prostate cancer, lung cancer, and esophageal cancer (3). However, [^11^C]choline has a high uptake in the liver, kidney, and spleen. An ^18^F-labeled choline analog was initially synthesized as [^18^F]fluoroethylcholine ([^18^F]FECh) to replace [^11^C]choline as a PET tracer due to the short physical half-life of ^11^C (20 min) (4). Although ^18^F has a longer half-life (110 min), [^18^F]FECh exhibited rapid accumulation in the urinary bladder, rendering it less desirable for imaging prostate cancer and pelvic lymph nodes. Therefore, [^18^F]fluorocholine (FCH (http://www.ncbi.nlm.nih.gov/books/NBK23563/#Choline18F)) was conceived to be a better biological analog than [^18^F]FECh (5). PET studies with FCH showed high uptake in malignancies in patients with prostate cancer, breast carcinoma, and brain tumors (6, 7). Choline is also metabolized by choline oxidase in competition with CHK to choline betaine, which cannot be phosphorylated by CHK. There is a large isotope effect for the oxidation of choline to choline betaine with deuterium substitution of hydrogen on the ethanol portion of choline (8). Therefore, deuterated analogs of FCH would result in increased in vivo stability and greater tumor accumulation. Smith et al. (9) performed biodistribution studies of [^18^F]fluoro-[1,2-^2^H_4_]choline ([^18^F]12c) in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (Choline (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=choline+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Choline kinase (http://www.ncbi.nlm.nih.gov/gene/1119))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Choline kinase (http://www.ncbi.nlm.nih.gov/omim/612395))
- Clinical trials (Fluorocholine (http://www.clinicaltrials.gov/ct2/results?term=fluorocholine))
- Drug information in FDA (Fluorocholine (http://google2.fda.gov/search?q=fluorocholine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20and%20synthesis)]

[^18^F]12c was prepared in a two-step reaction (9). [^18^F]Fluoromethyl tosylate was prepared by reaction of methylene ditosylate with [^18^F]KF/K_2_CO_3_ in acetonitrile/crown ether/water for 10–15 min at 100°C. [^18^F]Fluoromethyl tosylate was purified with high-performance liquid chromatography, with a radiochemical yield of 26 ± 3% (non–decay-corrected, n = 12). A solution of [^18^F]fluoromethyl tosylate and N,N-dimethyl-[1,2-^2^H_4_]-ethanolamine in dimethylformamide was heated for 20 min at 100°C. The overall radiochemical yield of [^18^F]12c based on [^18^F]KF was 10 ± 4% (non–decay-corrected, n = 5) with >99% radiochemical purity and a total synthesis time of 150 min. Specific activity of [^18^F]12c was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20in%20vitro)]

[^18^F]12c was ~80% intact after treatment for 1 h with potassium permanganate, which oxidizes choline to choline betaine (9). Conversely, only 40% of FCH was intact. In the presence of choline oxidase, [^18^F]12c was 29 ± 4% intact after treatment for 1 h, whereas only 11 ± 8% of FCH was intact. Therefore, [^18^F]12c is more stable than FCH against oxidation.

## Animal Studies

### Rodent Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20rodentia)]

In a murine HCT116 human colon xenograft model, ex vivo biodistribution patterns of [^18^F]12c and FCH were compared at 2, 30, and 60 min after injection (9). Tumor accumulation of [^18^F]12c was 0.6% injected dose/gram (ID/g), 1.7% ID/g, and 2.3% ID/g at 2, 30, and 60 min, respectively. On the other hand, tumor accumulation of FCH was 0.3% ID/g, 0.9% ID/g, and 1.2% ID/g at 2, 30, and 60 min, respectively. Therefore, [^18^F]12c exhibited ~1-fold higher accumulation in the tumors than FCH did at these time points. Little difference was observed in the biodistribution patterns in normal tissues with the two tracers, with prominent radioactivity in the kidney and liver. The plasma concentrations of both tracers were <0.1% ID/g at 2 min after injection, with <10% of FCH intact and ~50% of [^18^F]12c intact as predicted from the deuterium isotope effect.

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20primate%20NOT%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20human)]

No publication is currently available.

## References

1 Zeisel S.H., Blusztajn J.K. (1994). Choline and human nutrition. Annu Rev Nutr.
2 Podo F. (1999). Tumour phospholipid metabolism. NMR Biomed.
3 Hara T. (2002). 11C-choline and 2-deoxy-2-[18F]fluoro-D-glucose in tumor imaging with positron emission tomography. Mol Imaging Biol.
4 Hara T., Yuasa M. (1997). Automated synthesis of fluorine-18 labeled choline analogue: 2-fluoroetheyl-dimethyl-2-oxyethylammonium. J Nucl Med.
5 DeGrado T.R., Coleman R.E., Wang S., Baldwin S.W., Orr M.D., Robertson C.N., Polascik T.J., Price D.T. (2001). Synthesis and evaluation of 18F-labeled choline as an oncologic tracer for positron emission tomography: initial findings in prostate cancer. Cancer Res.
6 DeGrado T.R., Baldwin S.W., Wang S., Orr M.D., Liao R.P., Friedman H.S., Reiman R., Price D.T., Coleman R.E. (2001). Synthesis and evaluation of (18)F-labeled choline analogs as oncologic PET tracers. J Nucl Med.
7 Hara T., Kondo T., Hara T., Kosaka N. (2003). Use of 18F-choline and 11C-choline as contrast agents in positron emission tomography imaging-guided stereotactic biopsy sampling of gliomas. J Neurosurg.
8 Gadda G. (2003). pH and deuterium kinetic isotope effects studies on the oxidation of choline to betaine-aldehyde catalyzed by choline oxidase. Biochim Biophys Acta.
9 Smith G., Zhao Y., Leyton J., Shan B., Nguyen Q.D., Perumal M., Turton D., Arstad E., Luthra S.K., Robins E.G., Aboagye E.O. (2011). Radiosynthesis and pre-clinical evaluation of [(18)F]fluoro-[1,2-(2)H(4)]choline. Nucl Med Biol.